# Biphenyl-3-yl-4-[^11^C]methoxyphenylcarbamate

Chemical name: | Biphenyl-3-yl-4-[^11^C]methoxyphenylcarbamate
Abbreviated name: | [^11^C]-1
Synonym: | [^11^C]URB597-1
Agent category: | Compound
Target: | Fatty acid amide hydrolase (FAAH)
Target category: | Enzyme
Method of detection: | Positron emission tomography
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH)]

Fatty acid amide hydrolase (FAAH) is an integral membrane-bound serine hydrolase and a part of the endocannabinoid system (ECS), which comprises the cannabinoid receptors (CB1 and CB2), endogenous ligands termed endocannabinoids (anandamide and oleamide), transporters and enzymes (1, 2). FAAH plays a key role in the hydrolysis of a number of primary and secondary fatty acid amides, controlling the levels of the neuromodulatory endocannabinoids in the ECS (3, 4). FAHH is widely expressed in many tissues with the highest levels in the liver and brain (5). Genetic or pharmacological inactivation of FAAH in the brain leads to analgesic, anti-inflammatory, anxiolytic and anti-depression effects in animal models (6-8).

Cyclohexylcarbamic acid 3’-carbamoylbiphenyl-3-yl ester (URB597) is an irreversible, substrate-like inhibitor of FAAH involving carbamylation of the catalytic nucleophilic Ser^241^ and the O-biaryl group as the leaving group (9-11). Based on the structure of URB597, Wyffels et al. (12) prepared biphenyl-3-yl-4-[^11^C]methoxyphenylcarbamate ([^11^C]-1) for in vivo positron emission tomography (PET) imaging studies of the brain FAAH in mice. It was proposed that the carbamylation of Ser^241^ would leave the [^11^C]-methoxyanilino group bound to the FAAH for visualization of FAAH in the brain. However, the results of in vitro and ex vivo studies indicated that [^11^C]-1 is a reversible inhibitor of FAAH and the rapid brain washout of the tracer limits its utility as a PET agent for in vivo measurements of FAAH.

### Related Resource Links:

- Chapters in MICAD (FAAH (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=FAAH+AND+micad%5Bbook%5D))
- Gene information in NCBI (FAAH (http://www.ncbi.nlm.nih.gov/gene/2166))
- Articles in Online Mendelian Inheritance in Man (OMIM) (FAAH (http://omim.org/entry/602935))
- Clinical trials (FAAH (http://www.clinicaltrials.gov/ct2/results?term=FAAH&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20synthesis)]

Wyffels et al. (12) synthesized [^11^C]-1 by O-methylation of the desmethyl precursor biphenyl-3-yl-4-hydroxyphenylcarbamate with [^11^C]methyl iodide at 30°C for 10 min. Subsequent separation with high-performance liquid chromatography produced a radiochemical purity >99%. The radiochemical yield was 35 ± 9% based on [^11^C]methyl iodide and specific activity was 376 ± 135 GBq/μmol (10.2 ± 3.6 Ci/µmol; n = 7) at the end of synthesis. Total synthesis time, including HPLC purification was 40 min. The LogD value of [^11^C]-1 was 2.27 ± 0.07 (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20in%20vitro)]

Wyffels et al. (12) showed that compound 1 and URB597 inhibited the hydrolysis of [^3^H]-anandamide by hFAAH with IC_50_ values of 436 and 40 nM, respectively. Inhibition of hFAAH by compound 1 was reversible using dilution assay with the recovery of hFAAH activity, whereas URB597-treated hFAAH showed a slow recovery of the hFAAH activity upon dilution. Therefore, the inhibition mechanism of FAAH by compound 1 is different than that of URB597. Furthermore, in vitro metabolism studies using brain homogenates from C57BL/6J (wide-type) and FAAH^-/-^ mice revealed that [^11^C]-1 was >99% intact after incubation for 30 min at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20rodentia)]

Ex vivo biodistribution studies in C57BL/6J and FAAH^-/-^ mice (n = 3/group) were performed at 1, 10, 30, 60 and 90 min after intravenous injection of 3.7 MBq (0.1 mCi) [^11^C]-1(12). The distribution of radioactivity in the C57BL/6J and FAAH^-/-^ mice was highly similar. The accumulation levels in the brain were 8.6 ± 2.3% injected dose/gram (ID/g) and 8.3 ± 0.2% ID/g at 1 min, and 0.6 ± 0.2% ID/g and 0.7 ± 0.2% ID/g at 60 min in the C57BL/6J and FAAH^-/-^ mice, respectively. For the C57BL/6J mice, the liver accumulation decreased from 8.8 ± 4.2% ID/g at 1 min to 3.0 ± 0.2% ID/g at 90 min, whereas the highest accumulation in the small intestine was observed at 30 min (6.7 ± 1.5% ID/g) and slowly declined to 5.3 ± 2.1% ID/g at 90 min. The kidney and lung accumulation levels were about 10% ID/g at 1 min and 4.5% ID/g at 90 min. A slightly lower radioactivity levels in the liver, kidneys, and small intestine were observed in the FAAH^-/-^ mice as compared with the wide-type mice. [^11^C]-1 was ~10% intact in the plasma of the C57BL/6J mice at 10 min after injection with one polar metabolite. On the other hand, there were one additional polar metabolite was observed in the brains of both mice. [^11^C]-1 was 31 ± 9% and 55 ± 5% intact in the brain of the C57BL/6J and FAAH^-/-^ mice at 30 min after injection, respectively. The strong similarity of the metabolite profile of [^11^C]-1 in the wide-type mice to the profile in the FAAH^-/-^ mice suggests a non-FAAH-mediated metabolism of the tracer in vivo. In addition, a similar rapid washout of the tracer in both mice limits its utility as a PET agent for in vivo measurements of FAAH.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20human)]

No publication is currently available.

## References

1 Giang D.K., Cravatt B.F. (1997). Molecular characterization of human and mouse fatty acid amide hydrolases. Proc Natl Acad Sci U S A.
2 McKinney M.K., Cravatt B.F. (2005). Structure and function of fatty acid amide hydrolase. Annu Rev Biochem.
3 Bracey M.H., Hanson M.A., Masuda K.R., Stevens R.C., Cravatt B.F. (2002). Structural adaptations in a membrane enzyme that terminates endocannabinoid signaling. Science.
4 Egertova M., Giang D.K., Cravatt B.F., Elphick M.R. (1998). A new perspective on cannabinoid signalling: complementary localization of fatty acid amide hydrolase and the CB1 receptor in rat brain. Proc Biol Sci.
5 Thomas E.A., Cravatt B.F., Danielson P.E., Gilula N.B., Sutcliffe J.G. (1997). Fatty acid amide hydrolase, the degradative enzyme for anandamide and oleamide, has selective distribution in neurons within the rat central nervous system. J Neurosci Res.
6 Naidu P.S., Kinsey S.G., Guo T.L., Cravatt B.F., Lichtman A.H. (2010). Regulation of inflammatory pain by inhibition of fatty acid amide hydrolase. J Pharmacol Exp Ther.
7 Fowler C.J., Naidu P.S., Lichtman A., Onnis V. (2009). The case for the development of novel analgesic agents targeting both fatty acid amide hydrolase and either cyclooxygenase or TRPV1. Br J Pharmacol.
8 Bambico F.R., Duranti A., Tontini A., Tarzia G., Gobbi G. (2009). Endocannabinoids in the treatment of mood disorders: evidence from animal models. Curr Pharm Des.
9 Alexander J.P., Cravatt B.F. (2005). Mechanism of carbamate inactivation of FAAH: implications for the design of covalent inhibitors and in vivo functional probes for enzymes. Chem Biol.
10 Basso E., Duranti A., Mor M., Piomelli D., Tontini A., Tarzia G., Traldi P. (2004). Tandem mass spectrometric data-FAAH inhibitory activity relationships of some carbamic acid O-aryl esters. J Mass Spectrom.
11 Mor M., Rivara S., Lodola A., Plazzi P.V., Tarzia G., Duranti A., Tontini A., Piersanti G., Kathuria S., Piomelli D. (2004). Cyclohexylcarbamic acid 3'- or 4'-substituted biphenyl-3-yl esters as fatty acid amide hydrolase inhibitors: synthesis, quantitative structure-activity relationships, and molecular modeling studies. J Med Chem.
12 Wyffels L., Muccioli G.G., Kapanda C.N., Labar G., De Bruyne S., De Vos F., Lambert D.M. (2010). PET imaging of fatty acid amide hydrolase in the brain: synthesis and biological evaluation of an 11C-labelled URB597 analogue. Nucl Med Biol.